# ^68^Ga-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-p-Cl-Phe-cyclo(D-Cys-Tyr-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)D-Tyr-NH_2_

Chemical name: | ^68^Ga-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-p-Cl-Phe-cyclo(D-Cys-Tyr-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)D-Tyr-NH_2_
Abbreviated name: | ^68^Ga-DOTA-LM3
Synonym:
Agent category: | Peptide
Target: | Somatostatin receptor 2 (SSTR2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=47117741), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=71979669) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6750) for more information about somatostatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-LM3)]

Somatostatin (SSTR) is an inhibitor of the release of somatotropin, glucagon, insulin, gastrointestinal hormones, and other secretory proteins (1). SSTR is also known as somatotropin release-inhibiting factor (SRIF). SSTR is a cyclic polypeptide with two biologically active isoforms, SRIF-14 and SRIF-28, of 14 and 28 amino acids, respectively. SRIF has a short plasma half-life of <3 min (2). SSTR receptors (SSTRs) (G-protein–coupled) have been found on a variety of neuroendocrine tumors and cells of the immune system, and five individual subtypes (SSTR1–SSTR5) have been identified and subsequently cloned from animal and human tissues (3, 4). SST also inhibits cell proliferation and promotes apoptosis through binding to specific cell-surface SSTRs (5).

^111^In-Diethylenetriamine pentaacetic acid-octreotide (^111^In-DTPA-OCT) is an SST analog that, over the last decade, has remained the most widely used radiopharmaceutical and the only FDA approved radiotracer for the scintigraphic detection and staging of primary and metastatic neuroendocrine tumors bearing SSTRs with single-photon emission computed tomography (SPECT) (6). It has also shown promising results in peptide-receptor radionuclide therapy (7). Octreotide (OCT) is a cyclic peptide with eight amino acids. ^111^In-DTPA-OCT binds with high affinity to SSTR2 and SSTR5 and to SSTR3 to a lesser degree, but it does not bind to SSTR1 and SSTR4 (8). A large number of radiolabeled SST analogs have been reported using different radionuclides and different linkers. Currently used targeting SSTR peptides mainly are SSTR2 agonists. Therefore, there is a need for SSTR2 antagonist radioligands (9). p-Cl-Phe-cyclo(D-Cys-Tyr-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)D-Tyr-NH_2_ (LM3) is a novel selective SSTR2 antagonist. Fani et al. (10) prepared ^68^Ga-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-LM3 (^68^Ga-DOTA-LM3) as a positron emission tomography (PET) imaging agent for SSTR2.

### Related Resource Links:

- Chapters in MICAD (Somatostatin (http://www.ncbi.nlm.nih.gov/books?term=Somatostatin%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Somatostatin (http://www.ncbi.nlm.nih.gov/gene/6750), SSTR2 (http://www.ncbi.nlm.nih.gov/gene/6752))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Somatostain (http://omim.org/entry/182450), SSTR2 (http://omim.org/entry/182452))
- Clinical trials (Somatostatin receptor (http://www.clinicaltrials.gov/ct2/results?term=somatostatin+receptor))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-LM3+and+synthesis)]

DOTA-LM3 was synthesized via standard solid-phase peptide synthesis with a calculated mass of 1,522.0 Da in agreement with mass spectrometry (10). DOTA was incorporated at the N-terminus of the peptide. DOTA-LM3 was purified with high-performance liquid chromatography. ^68^Ga was complexed to DOTA-LM3 by reaction of DOTA-LM3 with ^64^Ga in sodium acetate (pH 4.0) for 8 min at 95°C. ^68^Ga-DOTA-LM3 had a >95% radiochemical purity and specific activity of 100 MBq/nmol (2.7 mCi/nmol) with a labeling yield >95%. ^68^Ga-DOTA-LM3 had a log D value of -2.13 ± 0.01 and a net charge of +1.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-LM3+and+in+vitro)]

Fani et al. (10) reported that ^nat^Ga-DOTA-LM3 had 50% inhibition concentration (IC_50_) values of >1,000, 12.5 ± 4.3, >1,000, >1,000, and >1,000 nM for human SSTR1, SSTR2, SSTR3, SSTR4, and SSTR5 receptors in competition with ^125^I-SRIF-28, respectively. Immunofluorescence studies showed that [Tyr^3^]octreotide (10 nM) triggers receptor internalization whereas ^nat^Ga-NODAGA-LM3 at a much higher concentration (1,000 nM) does not stimulate receptor internalization in HEK-sst2 cells. ^nat^Ga-DOTA-LM3 was able to inhibit receptor internalization induced by [Tyr^3^]octreotide.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-LM3+and+rodentia)]

Fani et al. (10) performed ex vivo biodistribution studies with 13.0 MBq (0.35 mCi) ^68^Ga-DOTA-LM3 in nude mice (n = 3) bearing HEK-sst2 xenografts of at 1 h after injection. The accumulation of radioactivity in the SSTR2 tumor was 28.72 ± 5.58% injected dose per gram (% ID/g). The kidney was the organ that had the highest accumulation (32.50% ID/g), followed by the lung (1.73% ID/g), bone (1.63% ID/g), stomach (1.08% ID/g), adrenal (1.06% ID/g), pancreas (0.91% ID/g), and liver (0.84% ID/g). Accumulation of radioactivity in the other tissues was low. The concentration in the blood was 1.21% ID/g. The tumor/blood, tumor/liver, tumor/kidney, and tumor/muscle ratios were 24.2, 34.3, 0.9, and 90.6, respectively. As a comparison, ^68^Ga-DOTA-LM3 accumulation in the kidney was 1-fold higher than ^64^Cu-NODAGA-LM3 at 1 h after injection with lower tumor/blood, tumor/kidney, and tumor/muscle ratios. Whole-body PET imaging visualized the SSTR2 tumor at 1 h after injection of 6 MBq (0.16 mCi) ^68^Ga-DOTA-LM3. The visualization was abrogated by co-injection of excess unlabeled peptide.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-LM3+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-LM3+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-LM3+and+human)]

No publication is currently available.

## References

1 Weckbecker G., Lewis I., Albert R., Schmid H.A., Hoyer D., Bruns C. (2003). Opportunities in somatostatin research: biological, chemical and therapeutic aspects. Nat Rev Drug Discov.
2 Patel Y.C., Wheatley T. (1983). In vivo and in vitro plasma disappearance and metabolism of somatostatin-28 and somatostatin-14 in the rat. Endocrinology.
3 Corleto V.D., Nasoni S., Panzuto F., Cassetta S., Delle Fave G. (2004). Somatostatin receptor subtypes: basic pharmacology and tissue distribution. Dig Liver Dis.
4 Moller L.N., Stidsen C.E., Hartmann B., Holst J.J. (2003). Somatostatin receptors. Biochim Biophys Acta.
5 Barnett P. (2003). Somatostatin and somatostatin receptor physiology. Endocrine.
6 Krenning E.P., Kwekkeboom D.J., Bakker W.H., Breeman W.A., Kooij P.P., Oei H.Y., van Hagen M., Postema P.T., de Jong M., Reubi J.C., et al. (1993). Somatostatin receptor scintigraphy with [111In-DTPA-D-Phe1]- and [123I-Tyr3]-octreotide: the Rotterdam experience with more than 1000 patients. Eur J Nucl Med.
7 Kwekkeboom D.J., Mueller-Brand J., Paganelli G., Anthony L.B., Pauwels S., Kvols L.K. (2005). M. O'Dorisio T, R. Valkema, L. Bodei, M. Chinol, H.R. Maecke, and E.P. Krenning, Overview of results of peptide receptor radionuclide therapy with 3 radiolabeled somatostatin analogs. J Nucl Med.
8 Storch D., Behe M., Walter M.A., Chen J., Powell P., Mikolajczak R., Macke H.R. (2005). Evaluation of [99mTc/EDDA/HYNIC0]octreotide derivatives compared with [111In-DOTA0,Tyr3, Thr8]octreotide and [111In-DTPA0]octreotide: does tumor or pancreas uptake correlate with the rate of internalization?. J Nucl Med.
9 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
10 Fani M., Del Pozzo L., Abiraj K., Mansi R., Tamma M.L., Cescato R., Waser B., Weber W.A., Reubi J.C., Maecke H.R. (2011). PET of somatostatin receptor-positive tumors using 64Cu- and 68Ga-somatostatin antagonists: the chelate makes the difference. J Nucl Med.